# ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-9-aminonanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-9-aminonanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ | [image]
Abbreviated name: | ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ | [image]
Synonym: | ^64^Cu-NO2A-(X)-BBN(7-14)NH_2_ | [image]
Agent Category: | Peptides | [image]
Target: | Gastrin-releasing peptide receptors (GRPR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^64^Cu | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of Cu-NO2A-(9-Anc)-BBN(7-14)NH_2_ by Lane et al (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging)]

^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid (NO2A)-9-aminonanoic acid (9-Anc)-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (BBN(7–14)NH_2_), abbreviated as ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_, is a bombesin (BBN)-based, ^64^Cu-NO2A-conjugated peptide that was synthesized by Lane et al. for use in positron emission tomography (PET) of tumors expressing gastrin-releasing peptide receptor (GRPR) (1, 2).

GRPR is a glycosylated G-protein–coupled receptor that is normally expressed in non-neuroendocrine tissues of the breast and pancreas and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (3, 4). GRPR has been found to be overexpressed in various human tumors, and a large number of BBN analogs have been investigated for GRPR-targeted imaging and therapy (5, 6). These analogs have been synthesized on the basis of either truncated BBN (BBN(6–14) or BBN(7–14)) or full-length BBN(1–14) (7, 8). Chelators and spacers have been used frequently for chelating metals and for improving the kinetics of conjugates (9-11).

^64^Cu is a radiometal with potential applications in diagnostic and therapeutic nuclear medicine. The half-life for ^64^Cu (t_1/2_ = 12.7 h) is long enough for drug preparation, quality control, imaging, and therapy (12, 13). However, use of ^64^Cu is limited by issues of in vivo transchelation to proteins found in blood and liver (such as superoxide dismutase) (1). A variety of chelators have been investigated for the purpose of stably chelating ^64^Cu (13). In general, ^64^Cu-labeled 1,4,7,10-tetraazacyclodecane-1,4,7,10-tetraacetic acid (^64^Cu-DOTA) and ^64^Cu-labeled 1,4,8,11-tetraazacyclotetradecane-1,4,8,11-tetraacetic acid (^64^Cu-TETA) exhibit high uptake and retention in nontarget organs, which limits their application. Cross-bridged (CB) analogs, such as CB-DO2A ((1,4,7,10-tetraazabicyclo[5.5.2]tetradecane-4,10-diyl)diacetic acid), CB-TE2A ((1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-4,11-diyl)diacetic acid), SarAr (1-N-(4-aminobenzyl)-3,6,10,13,16,19-hexa-aza-bicyclo-[6.6.6]eichosane-1,8-diamine), and NOTA (1,4,7-triazacyclononane-1,4,7-triacetic acid), demonstrate improved copper containment by enhancing the ligand's rigidity (2, 14).

Prasanphanich et al. recently reported that the NOTA-based ^64^Cu-NOTA-8-Aoc-BBN(7–14)NH_2_ (http://www.ncbi.nlm.nih.gov/books/NBK23504/) conjugate (where 8-Aoc = 8-aminooctanoic acid) exhibited decreased accumulation in hepatic tissue as compared with other chelator-based (DOTA, TETA, and CB-TE2A) conjugates (2, 14). To improve the tumor uptake and maintain the good pharmacokinetic properties of the ^64^Cu-NOTA-8-Aoc-BBN(7–14)NH_2_ conjugate, Lane et al. synthesized a new group of conjugates with the NOTA derivative NO2A and replaced the spacer 8-Aoc with an aliphatic or aromatic linking (1). These conjugates were abbreviated as ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_, where X denotes the pharmacokinetic modifier, such as AMBA (para-aminobenzoic acid), β-Ala (beta-alanine), 5-Ava (5-aminovaleric acid), 6-Ahx (6-aminohexanoic acid), 8-Aoc, and 9-Anc. The β-Ala, 5-Ava, 6-Ahx, and 9-Anc are aliphatic pharmacokinetic modifiers, ranging from three to nine carbons in length, whereas AMBA is an aromatic pharmacokinetic modifier and is more rigid than the aliphatic modifiers. Evidence indicates that a spacing moiety, ranging from three to eight carbons in length, can assist in receptor-mediated uptake (15). Conjugates containing an aromatic linker have significantly higher uptake and retention in PC-3 tumor tissue than those containing hydrocarbon or ether linkers (15, 16). Studies by Lane et al. have shown that the spacer X in the ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates has a significant role in clearance, accumulation, and retention of the conjugates in tumor tissue (1). The four conjugates showing the most favorable pharmacokinetic properties and the highest degree of pancreas and tumor accumulation were those in which X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA. PET imaging with these conjugates produced high-contrast images of PC-3 tumor xenografts in severe combined immunodeficient (SCID) mice (1). This chapter describes the data obtained with ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_. Detailed information for other ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates is available in MICAD (http://www.ncbi.nlm.nih.gov/books/NBK5330/) (1).

### Related Resource Links:

- Protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) information for GRPR
- Structure information of BN and analogs in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=bombesin)
- GRPR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=GRPR%20AND%20micad%5bbook%5d)
- Chapter on ^64^Cu-NO2A-8-Aoc-BBN(7–14)NH_2_ (http://www.ncbi.nlm.nih.gov/books/NBK23504/) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

Lane et al. described the synthesis of ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates in detail (1). For ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_, the peptide 9-Anc-BBN(7–14)NH_2_ was synthesized with traditional F-moc chemistry. Crude peptides were obtained in ~60% yield. NOTA was conjugated to the peptide via an active ester to produce the NOTA derivative conjugate, NO2A-(9-Anc)-BBN(7–14)NH_2_, with ~80% yield after purification. The calculated and observed molecular weights for the NO2A-(9-Anc)-BBN peptide conjugate were both 1,380.7. ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ was synthesized with the reaction of ^64^CuCl_2_ and peptide conjugate in the presence of ammonium acetate. The radiochemical yield was >90%. All of the unconjugated peptide precursors, peptide conjugates, and metallated peptide conjugates were purified with reverse-phase high-performance liquid chromatography (RP-HPLC) and characterized with mass spectrometry. The radiochemical purity and specific activity were not described.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

The stability of ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ in human serum albumin was determined with quantification of the ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ peak area in the radiometric RP-HPLC chromatogram. The percent of intact conjugate was >80% after 24 h incubation (37°C, 5% CO_2_-enriched atmosphere) with human serum albumin (1).

A competitive displacement binding assay was performed in PC-3 cells with ^125^I-(Tyr^4^)-BBN as the radioligand (1). High binding affinities were observed for both unlabeled NO2A-(9-Anc)-BBN(7–14)NH_2_ (inhibition constant (K_i_) = 1.99 ± 0.17 nM) and ^nat^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ (^nat^Cu = natural copper) (K_i_ = 6.75 ± 1.70 nM).

Internalization was determined after incubation of the PC-3 cells with ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ for different times. Externalization was determined after an initial 40-min internalization period in PC-3 cells followed by washing the cells. The results revealed GRPR-mediated trapping of radioactivity inside the cells with very little externalization of ^64^Cu with cells washed after the internalization period (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

Biodistribution studies of ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ were performed in both normal CF-1 mice (n = 4 or 5/group) and PC-3 xenograft-bearing SCID mice (n = 5 mice/group per time point). The biodistribution data were compared among the ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates (where X = β-Ala, 5-Ava, 6-Ahx, 8-Aoc, 9-Anc, or AMBA) (1, 2).

In normal mice, rapid clearance from blood was observed for all conjugates, with ≤0.5% injected dose per gram tissue (% ID/g) remaining in circulation at 1 h after injection (for ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_, 0.5 ± 0.20% ID/g). Excretion properties of the conjugates were directly related to the length of X. Increasing the hydrophobicity of the conjugate (increasing the aliphatic length of X) led to higher excretion rates via the hepatobiliary system. The hepatic accumulation at 1 h after injection ranged from 0.70% ID/g (where X = AMBA) to 2.35% ID/g (where X = 9-Anc). Uptake of the conjugates in GRPR-expressing pancreas ranged from 15.10 to 30.63% ID/g at 1 h after injection, with 22.80 ± 2.96% ID/g for ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_, indicating effective GRPR targeting for the radiolabeled conjugates. The four conjugates showing the most favorable pharmacokinetic properties and the highest degree of pancreas accumulation were those in which X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA, which were further studied in PC-3 tumor-bearing SCID mice (1).

In tumor-bearing SCID mice, all four conjugates were cleared effectively from the bloodstream, with 0.93–1.35% ID/g remaining at 1 h after injection (for ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_, 1.04 ± 0.25% ID/g). Excretion routes were similar to those observed in normal CF-1 mice, with more hydrophobic conjugates excreted through the hepatobiliary system. Minimal accumulation of radioactivity was observed in the liver at 24 h, ranging from 0.68 (where X = 8-Aoc) to 1.37% ID/g (where X = 9-Anc), suggesting that the metal complex was effectively stable under in vivo conditions. High receptor-mediated accumulation was observed in both the pancreas and tumor for all conjugates. Radioactivity uptake values for ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ at 1 h, 4 h, and 24 h after injection were 3.73 ± 1.23, 0.99 ± 0.26, and 0.62 ± 0.10% ID/g, respectively, in the tumor; 20.76 ± 4.24, 4.03 ± 1.07, and 1.20 ± 0.15% ID/g, respectively, in the pancreas; and 6.77 ± 1.76, 1.66 ± 0.92, and 0.77 ± 0.27% ID/g, respectively, in the kidney (1).

PET imaging was performed at 18 h after tail-vein injection of ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ (where X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA) (1). The PC-3 tumors were clearly identifiable in PET images for all conjugates. Tumor/background ratios decreased with increased length of X, which appears to be a function of increasing the hydrophobicity of the conjugate. ^64^Cu-NO2A-(9-Anc)-BBN(7–14)NH_2_ demonstrated moderate tumor uptake with significant abdominal accumulation (liver and gastrointestinal tract). In comparison, for ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = AMBA, superior tumor uptake with minimal liver accumulation was observed. For ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = 8-Aoc, high tumor and liver uptake values were observed. For ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = 6-Ahx, high tumor uptake as well as relatively high kidney accumulation were observed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Lane S.R., Nanda P., Rold T.L., Sieckman G.L., Figueroa S.D., Hoffman T.J., Jurisson S.S., Smith C.J. (2010). Optimization, biological evaluation and microPET imaging of copper-64-labeled bombesin agonists, [64Cu-NO2A-(X)-BBN(7-14)NH2], in a prostate tumor xenografted mouse model. Nucl Med Biol.
2 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Erspamer V., Erpamer G.F., Inselvini M. (1970). Some pharmacological actions of alytesin and bombesin. J Pharm Pharmacol.
5 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
6 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
7 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
8 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
9 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
10 Mu L., Honer M., Becaud J., Martic M., Schubiger P.A., Ametamey S.M., Stellfeld T., Graham K., Borkowski S., Lehmann L., Dinkelborg L., Srinivasan A. (2010). In vitro and in vivo characterization of novel 18F-labeled bombesin analogues for targeting GRPR-positive tumors. Bioconjug Chem.
11 Becaud J., Mu L., Karramkam M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Lehmann L., Borkowski S., Berndorff D., Dinkelborg L., Srinivasan A., Smits R., Koksch B. (2009). Direct one-step 18F-labeling of peptides via nucleophilic aromatic substitution. Bioconjug Chem.
12 Wadas T.J., Wong E.H., Weisman G.R., Anderson C.J. (2007). Copper chelation chemistry and its role in copper radiopharmaceuticals. Curr Pharm Des.
13 Hoffman T.J., Smith C.J. (2009). True radiotracers: Cu-64 targeting vectors based upon bombesin peptide. Nucl Med Biol.
14 Prasanphanich A.F., Nanda P.K., Rold T.L., Ma L., Lewis M.R., Garrison J.C., Hoffman T.J., Sieckman G.L., Figueroa S.D., Smith C.J. (2007). [64Cu-NOTA-8-Aoc-BBN(7-14)NH2] targeting vector for positron-emission tomography imaging of gastrin-releasing peptide receptor-expressing tissues. Proc Natl Acad Sci U S A.
15 Smith C.J., Gali H., Sieckman G.L., Higginbotham C., Volkert W.A., Hoffman T.J. (2003). Radiochemical investigations of (99m)Tc-N(3)S-X-BBN[7-14]NH(2): an in vitro/in vivo structure-activity relationship study where X = 0-, 3-, 5-, 8-, and 11-carbon tethering moieties. Bioconjug Chem.
16 Garrison J.C., Rold T.L., Sieckman G.L., Naz F., Sublett S.V., Figueroa S.D., Volkert W.A., Hoffman T.J. (2008). Evaluation of the pharmacokinetic effects of various linking group using the 111In-DOTA-X-BBN(7-14)NH2 structural paradigm in a prostate cancer model. Bioconjug Chem.